# 1-[^18^F]Fluoro-3,6-dioxatetracosane

Chemical name: | 1-[^18^F]Fluoro-3,6-dioxatetracosane
Abbreviated name: | [^18^F]SteP2
Synonym: | [^18^F]7a
Agent Category: | Compound
Target: | Liposomes
Target Category: | Non-targeted
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=liposomes)]

Liposomes may be characterized as artificial vesicle-like structures possessing an inner hydrophilic core surrounded by one or more outer hydrophobic bilayer membrane(s) that are composed of various natural or synthetic lipids, including phospholipids (1). Liposomes are used as drug delivery vehicles because the hydrophilic core can entrap a variety of compounds such as anti-cancer, anti-fungal, or photoactive drugs, or even nucleic acids and their derivatives for gene therapy (2-4). Therefore, it is important to evaluate the distribution of these drug delivery vesicles in an in vivo system using a non-invasive technique. 2-[^18^F]-2-Deoxy-2-fluoroglucose has been used to investigate the in vivo biodistribution of liposomes in tumor-bearing mice with the use of photon emission tomography (PET), but the synthesis of these labeled liposomes was inefficient and required much handling by the operator (5). More recently, Marik et al. investigated the biodistribution of liposomes encapsulating [^18^F]fluorodipalmitin, but the method used to generate the labeled liposomes is not suitable to label preformed liposomes (6). Urakami and colleagues developed a solid-phase transition method to generate a novel ^18^F-labeled probe, 1-[^18^F]fluoro-3,6-dioxatetracosane ([^18^F]SteP2 or [^18^F]7a), which can be used in a single-step process for the rapid labeling of preformed liposomes, and the investigators used PET to study the biodistribution of [^18^F]SteP2 in normal mice (7). In another study, the distribution of [^18^F]SteP2-labeled, liposome-encapsulated hemoglobin (LEH) in rat brains under ischemic conditions was investigated by Urakami and colleagues (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of [^18^F]SteP2 was described by Urakami and colleagues (7). Briefly, compound 7a was prepared from the corresponding alcohol of 3,6-dioxatetracosane using (diethylamino)sulfur fluoride (7). The agent was labeled with [^18^F] using a nucleophilic substitution reaction by refluxing the sulfonate of compound 7a with a mixture of [^18^F]potassium fluoride, 4,7,13,16,21,24-Bexaoxa-1,10-diazabicyclo[8,8,8]hexacosane, and acetonitrile using a method modified from that of Harada et al. (9) as described by Urakami and colleagues (7). The radiochemical yield, purity, storage conditions, and specific activity of [^18^F]SteP2 were not reported.

Liposomes of three different sizes (90, 170, and 570 nm) were labeled with [^18^F]SteP2 by the solid-phase transition method (7). To achieve this, [^18^F]SteP2 was dried into a thin film in a test tube. The three different liposomes were respectively added to the dried compound at a molar ratio of 100:1 (lipid:[^18^F]SteP2) and incubated for 15 min at 65°C. The labeled liposomes were ultracentrifuged to remove any unincorporated [^18^F]SteP2, and the various fractions (labeled liposomes, supernatant, and any precipitate) were quantified with high-performance liquid chromatography. On the basis of four separate determinations, the liposome labeling efficiency with [^18^F]SteP2 was ~85%.

The stability of [^18^F]SteP2-labeled liposomes was determined by exposing them to 50% fetal bovine serum for 1 h at 37°C (7). Under these conditions, amphiphilic compounds such as [^18^F]SteP2 that are incorporated to the lipid bilayer through weak hydrophobic interactions are known to transfer from the liposome to the high-density lipoproteins present in the serum. The liposomes and the lipoproteins in the serum were fractionated with gel filtration chromatography, and the amount of label remaining bound to the liposomes was determined. Under these experimental conditions, ~90% of the label was reported to be bound to the liposomes.

In another study, [^18^F]SteP2-labeled LEH was prepared and labeled using the procedures described above (8). Labeling efficiency for LEH was reported to be 46.4 ± 4.8%, but the radiochemical purity, stability, and specific activity of [^18^F]SteP2 LEH were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=118F+fluoro+3+6+dioxatetracosane+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=118F+fluoro+3+6+dioxatetracosane+rodentia)]

The biodistribution of [^18^F]SteP2-labeled liposomes of different sizes was studied in normal mice (7). The animals (number of animals per group was not reported) were respectively injected with free [^18^F]SteP2 and the labeled liposomes through the tail vein. Whole-body imaging of the injected animals was performed at various time points between 1 and 60 min after the injection. Whole-body imaging showed that the larger the size of the labeled liposome, the higher the radioactivity that accumulated in the spleen. With free [^18^F]SteP2, the radioactivity accumulated primarily in the kidneys immediately after the injection and was subsequently excreted in the urine.

To investigate accumulation of the labeled liposomes in various organs of the animals, the mice were euthanized after imaging, and the radioactivity accumulated in all the major organs was determined. This study revealed that radioactivity from free [^18^F]SteP2 and the labeled liposomes had accumulated mainly in the blood (~25% of injected dose/gram tissue (% ID/g)), liver (~20% ID/g), spleen (10–15% ID/g), and kidneys (~2.5% ID/g) at 60 min after administration of the radiotracers.

In another study, Urakami and colleagues investigated the distribution of [^18^F]SteP2-labeled LEH in rat brains under ischemic conditions (8). To confirm absence of blood flow in the ischemic region of the rat brains under in vivo conditions, imaging was performed after the administration of radioactive oxygen–labeled water. Twenty minutes after the ischemic conditions were confirmed, the animals were injected with labeled LEH and dynamic imaging was performed continuously for the next 60 min. Initially, little signal was observed in the ischemic brain area; however, during the next 60 min the radioactivity gradually increased in the cerebral cortex, but no detectable signal was obtained from the basal ganglia ischemic core, which indicated that, compared with the basal ganglia, the cerebral cortex was selectively protected. With results obtained from these studies, the investigators concluded that PET imaging could be used to investigate the distribution of [^18^F]SteP2-labeled, liposome-encapsulated drugs in small animals (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+SteP2+Non+Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+SteP2+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+SteP2+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Immordino M.L., Dosio F., Cattel L. (2006). Stealth liposomes: review of the basic science, rationale, and clinical applications, existing and potential. Int J Nanomedicine.
2 Aigner A. (2008). Cellular delivery in vivo of siRNA-based therapeutics. Curr Pharm Des.
3 Gershkovich P., Wasan K.M., Barta C.A. (2008). A review of the application of lipid-based systems in systemic, dermal/ transdermal, and ocular drug delivery. Crit Rev Ther Drug Carrier Syst.
4 Wang Y., Saad M., Pakunlu R.I., Khandare J.J., Garbuzenko O.B., Vetcher A.A., Soldatenkov V.A., Pozharov V.P., Minko T. (2008). Nonviral nanoscale-based delivery of antisense oligonucleotides targeted to hypoxia-inducible factor 1 alpha enhances the efficacy of chemotherapy in drug-resistant tumor. Clin Cancer Res.
5 Oku N., Tokudome Y., Tsukada H., Kosugi T., Namba Y., Okada S. (1996). In vivo trafficking of long-circulating liposomes in tumour-bearing mice determined by positron emission tomography. Biopharm Drug Dispos.
6 Marik J., Tartis M.S., Zhang H., Fung J.Y., Kheirolomoom A., Sutcliffe J.L., Ferrara K.W. (2007). Long-circulating liposomes radiolabeled with [18F]fluorodipalmitin ([18F]FDP). Nucl Med Biol.
7 Urakami T., Akai S., Katayama Y., Harada N., Tsukada H., Oku N. (2007). Novel amphiphilic probes for [18F]-radiolabeling preformed liposomes and determination of liposomal trafficking by positron emission tomography. J Med Chem.
8 Urakami T., Kawaguchi A.T., Akai S., Hatanaka K., Koide H., Shimizu K., Asai T., Fukumoto D., Harada N., Tsukada H., Oku N. (2009). In vivo distribution of liposome-encapsulated hemoglobin determined by positron emission tomography. Artif Organs.
9 Harada N., Ohba H., Fukumoto D., Kakiuchi T., Tsukada H. (2004). Potential of [(18)F]beta-CFT-FE (2beta-carbomethoxy-3beta-(4-fluorophenyl)-8-(2-[(18)F]fluoroethyl)nortrop ane) as a dopamine transporter ligand: A PET study in the conscious monkey brain. Synapse.